# Arginine-glycine-aspartic acid peptide-labeled quantum dot 705

Chemical name: | Arginine-glycine-aspartic acid peptide-labeled quantum dot 705
Abbreviated name: | QD705-RGD
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal/contrast: | Quantum dot 705 (QD705)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=QD705-RGD%20OR%20RGD-labeled%20quantum%20dots)]

Arginine-glycine-aspartic acid peptide-labeled quantum dot 705 (QD705-RGD) is an integrin-targeted molecular imaging agent developed for near-infrared (NIR) optical imaging of tumor vasculature (1). QD705 has an emission maximum at 705 nm.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiologic processes. These processes are governed at both the extracellular and intracellular levels by several factors (2, 3). Among the molecules that regulate angiogenesis are integrins, a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5).These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Some integrins recognize a single ECM protein ligand, whereas some can bind several ligands. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Integrin α_v_β_3_ receptor expression on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue but is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly up-regulated in certain types of tumor cells and in almost all tumor vasculature. Increased levels of integrin α_v_β_3_ expression are closely associated with increased cell invasion and metastasis. Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (1, 6).

Optical imaging is an imaging method that utilizes light photons emitted from bioluminescence and fluorescence probes. Fluorescence imaging in the visible light range of 395-600 nm can penetrate only to a depth of 1-2 cm and has significant background signal because of tissue autofluorescence. NIR (700-900 nm) fluorescence imaging has the advantages of relatively higher tissue penetration and lower autofluorescence from non-target tissue (6). Quantum dots (QDs) are colloidal semiconductor nanocrystals with very high levels of brightness and photostability, high molar extinction coefficients, and broad absorption with narrow and symmetric photoluminescence spectra spanning the ultraviolet to NIR (7, 8). Their fluorescent emission can be size-tuned as a function of core size. The best QD fluorophores are mostly made of cadmium selenide (CdSe) cores overcoated with a layer of ZnS (9). The potential toxicity of QDs is not well established. Not all QDs are alike, and their toxicity appears to depend on multiple physicochemical factors (10). Studies have shown a concentration-dependent in vitro cytotoxicity of CdSe QDs under certain conditions, and this toxicity appears to be significantly reduced by coating (11-13). The surfaces of QDs can be modified to be water soluble and biocompatible, and QDs can be attached to targeting molecules such as antibodies and peptides. Cai et al. (1) developed the first RGD peptide-labeled QDs for imaging of integrin α_v_β_3_-positive tumor vasculature.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28QD705-RGD%20OR%20RGD-labeled%20quantum%20dots%29%20AND%20synthesis)]

Cai et al. (1, 14) reported the synthesis of QD705-RGD using commercially available amine-modified QD705 (emission maximum, 705 nm). A detailed protocol was described by Cai et al. (14). Briefly, these QDs were built with a polyethylene glycol spacer (molecular weight 2,000) covalently attached to the QD705 surface. QD705 was first conjugated to a heterobifunctional cross-linker, 4-maleimidobutyric acid N-hydroxysuccinimide ester, to yield a maleimide-nanocrystal surface (maleimide-QD705). The lysine є-amino group of a potent integrin α_v_β_3_ antagonist, c(RGDyK), was reacted with S-acetylthioglycolic acid N-hydroxysuccinimide ester. This was followed by thiol deprotection by hydroxylamine under neutral condition to yield the thiolated RGD peptide, c(RGDy(є-acetylthiol)K) (RGD-SH). The maleimide-QD705 was reacted with RGD-SH for 1 h at pH 7.5. The final QD705-RGD was purified by size-exclusion chromatography. It was estimated that there were 30-50 RGD peptides per QD with a ligand coupling efficiency of 40-50%. Atomic force microscopy revealed discrete entities with smooth and uniform surface features, vertical heights of 5-7 nm, and lateral sizes of 15-20 nm. These results indicated that the structures were single QDs and that the preparation produced monodisperse single QD705-RGD particles without aggregation. These findings were confirmed by scanning electron microscopy.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28QD705-RGD%20OR%20RGD-labeled%20quantum%20dots%29%20AND%20in%20vitro)]

Cai et al. (1) determined the in vitro binding affinity of QD705-RGD in live and fixed MCF-7 (integrin α_v_β_3_-negative human breast cancer cell line), MDA-MB-435 (human breast cancer cell line with medium integrin α_v_β_3_-positive expression), and U87MG (human glioblastoma with high integrin α_v_β_3_ expression) cells. These cells were blocked with 0.1% bovine serum albumin, stained, and examined under the microscope. QD705-RGD did not bind to MCF-7 (integrin-negative) cells. The integrin-positive cells (MDA-MB-435 and U87MG) were clearly visualized in fluorescence images from QD705-RGD binding. The fluorescence intensity correlated with the integrin expression level of the cell lines. This binding was blocked effectively by 2 μM c(RGDyK). Unconjugated QD705 showed no significant binding to any of the cell lines.

Ex vivo tumor tissue binding studies were performed by Cai et al. (1). Tumor tissues generated from MCF-7, MDA-MB-435, and U87MG cells were cryosectioned at –20 °C into 8-μm slices, which were fixed in cold acetone and then stained with either QD705 or QD705-RGD. The results were similar to those of in vitro cell binding. QD705 had minimal nonspecific binding to all tumor tissues. QD705-RGD showed high binding to the U87MG tumor tissue but no binding to the MCF-7 tumor tissue.

Cai et al. (1) incubated QD705 and QD705-RGD in complete mouse serum at 37 °C to evaluate the change in fluorescent signal as a function of time. Fluorescence signal intensity decreased significantly over time for both QDs. After 24 h of incubation, the intensity decreased to 73.6% and 66.4% of the original values for QD705 and QD705-RGD, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28QD705-RGD%20OR%20RGD-labeled%20quantum%20dots%29%20AND%20rodentia)]

Cai et al. (1) performed in vivo distribution and imaging studies of QD705-RGD in athymic nude mice bearing U87MG tumors on their shoulders (tumor size, 0.5-0.8 cm^3^). Each mouse was administered i.v. QD705 or QD705-RGD (200 pmol of QDs, 6-10 nmol of peptide). The mice were imaged by an optical system with a custom-designed, spectrally optimized lens system. With QD705-RGD, a fluorescence signal was observed in the tumor as early as 20 min after injection. The tumor signal intensity reached a maximum at 6 h. The tumor/background ratios (n = 3) were 3.08 ± 1.42, 3.39 ± 1.13, 4.42 ± 1.88, and 2.09 ± 1.17 at 1, 4, 6, and 27 h after injection, respectively. With QD705, no significant fluorescent signal was observed in the tumor at all time points. Both QD705 and QD705-RGD accumulated rapidly in the liver, spleen, bone marrow, and lymph nodes. Uptake in the liver was observed as early as 10 min after injection. The liver signal from QD705-RGD was slightly lower than that of QD705. The authors suggested that the difference might be caused by the overall charge difference between QD705 and QD705-RGD. On the basis of these results, mice were euthanized at 6 h after injection, and the tumors were harvested and imaged immediately. The U87MG tumors from QD705-RGD mice showed clear signal intensity, but no signal was observed in tumors from QD705 mice. The signal from the QD705-RGD tumors was heterogeneous, and the authors suggested that the signal came mainly from the tumor vasculature. Microscope images of tumor cryosections confirmed that QD705-RGD did not extravasate and remained within the tumor vasculature.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28QD705-RGD%20OR%20RGD-labeled%20quantum%20dots%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28QD705-RGD%20OR%20RGD-labeled%20quantum%20dots%29%20AND%20non-human%20primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28QD705-RGD%20OR%20RGD-labeled%20quantum%20dots%29%20AND%20human)]

No publication is currently available.

## NIH Support

NCI R21 CA102123, NIBIB R21 EB001785, NCI SAIRP R24 CA93862.

## References

1. Cai, W., D.W. Shin, K. Chen, O. Gheysens, Q. Cao, S.X. Wang, S.S. Gambhir, and X. Chen, Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett, 2006. 6(4): p. 669-76.

2. Jin, H. and J. Varner, Integrins: roles in cancer development and as treatment targets. Br J Cancer, 2004. 90(3): p. 561-5.

3. Paulhe, F., S. Manenti, L. Ysebaert, R. Betous, P. Sultan, and C. Racaud-Sultan, Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des, 2005. 11(16): p. 2119-34.

4. Hood, J.D. and D.A. Cheresh, Role of integrins in cell invasion and migration. Nat Rev Cancer, 2002. 2(2): p. 91-100.

5. Hwang, R. and J. Varner, The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am, 2004. 18(5): p. 991-1006, vii.

6. Massoud, T.F. and S.S. Gambhir, Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev, 2003. 17(5): p. 545-80.

7. Lim, Y.T., S. Kim, A. Nakayama, N.E. Stott, M.G. Bawendi, and J.V. Frangioni, Selection of quantum dot wavelengths for biomedical assays and imaging. Mol Imaging, 2003. 2(1): p. 50-64.

8. Michalet, X., F.F. Pinaud, L.A. Bentolila, J.M. Tsay, S. Doose, J.J. Li, G. Sundaresan, A.M. Wu, S.S. Gambhir, and S. Weiss, Quantum dots for live cells, in vivo imaging, and diagnostics. Science, 2005. 307(5709): p. 538-44.

9. Medintz, I.L., H.T. Uyeda, E.R. Goldman, and H. Mattoussi, Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater, 2005. 4(6): p. 435-46.

10. Hardman, R., A toxicologic review of quantum dots: toxicity depends on physicochemical and environmental factors. Environ Health Perspect, 2006. 114(2): p. 165-72.

11. Lovric, J., H.S. Bazzi, Y. Cuie, G.R. Fortin, F.M. Winnik, and D. Maysinger, Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med, 2005. 83(5): p. 377-85.

12. Shiohara, A., A. Hoshino, K. Hanaki, K. Suzuki, and K. Yamamoto, On the cyto-toxicity caused by quantum dots. Microbiol Immunol, 2004. 48(9): p. 669-75.

13. Derfus, A.M., W.C.W. Chan, and S.N. Bhatia, Probing the cytotoxicity of semiconductor quantum dots. Nano Letters, 2004. 4(1): p. 11-18.

14. Cai, W. and X. Chen, Preparation of peptide-conjugated quantum dots for tumor vasculature-targeted imaging. Nat Protoc, 2008. 3(1): p. 89-96.